# (R,S)-2-(N-Propyl-N-1'-[^11^C]-propyl)amino-5-hydroxytetralin

Chemical name: | (R,S)-2-(N-Propyl-N-1'-[^11^C]-propyl)amino-5-hydroxytetralin
Abbreviated name: | [^11^C]-5-OH-DPAT
Synonym:
Agent Category: | Compound
Target: | D_2_ and D_3_ dopamine receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five dopamine receptor subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_). D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. Most striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein–coupled receptors and exist in high- and low-affinity states with respect to agonist binding. The two states are interconvertible. In the high-affinity state, dopamine receptors are coupled to G-proteins, whereas in the low-affinity state they are not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiologic conditions, dopamine is expected to bind predominately to receptors in the high-affinity state. The high-affinity state was suggested to be the functional form of the dopamine receptors (6).

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2/3_ receptors, making studies of extrastriatal D_2/3_ receptors difficult (7-9). In binding studies, [^123^I]epidepride was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2/3_ receptors (10). Epidepride exhibits marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (11), and in positron emission tomography (PET) in vivo studies (12-15) it identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguishes between the high- and low-affinity states of the D_2_ receptors. Many effects have been pursued to develop radiolabeled agonists for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain. (–)-N-[^11^C]Propyl-norapomorphine ([^11^C]NPA) and [^11^C](+)-4-N-propyl-,3,4a,5,6,10b-hexahydro-2H-naphth[1,2-b][1,4]oxazin-9-ol ([^11^C]PHNO) have been studied as radiolabeled dopamine agonists.

Various hydroxytetralin analogs with different binding affinities for the D_2_ receptors have been evaluated as agonist radiotracers (16). (R,S)-2-(N-Propyl-N-1'-[^11^C]-propyl)amino-5-hydroxytetralin ([^11^C]5-OH-DPAT) is being developed as a PET agent for the high-affinity state of D_2/3_ receptors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes%20and%20synthesis)]

Shi et al. (16) reported a two-step synthesis of [^11^C]5-OH-DPAT, in which [^11^C]propionyl chloride was reacted with 5-hydroxy-2-(N-propylamino)tetralin and followed by LiAlH_4_ reduction, with a radiochemical yield of 5–10% (based on [^11^C]CO_2_ at the end of bombardment and an average specific activity of 9–37 GBq/μmol (250–1,000 mCi/μmol) at end of synthesis after purification by high-performance liquid chromatography. [^11^C]Propionyl chloride was prepared by reacting [^11^C]CO_2_ with ethylmagnesium bromide, followed by reaction with phthaloyl chloride. The total synthesis time was 60–75 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes%20and%20in%20vitro)]

In a binding study of dopamine receptors in membranes of the rat striata with [^3^H]spiperone, 5-OH-DPAT had an inhibitory concentration (IC_50_) of 2.5 nM (16). In vitro autoradiography studies of rat brain slices indicated selective binding of [^11^C]5-OH-DPAT to the striata, which was completely inhibited by co-incubation with 10 μM sulpiride (a D_2/3_ antagonist) and Gpp(NH)p (conversion of the high-affinity state to the low-affinity state) (17). There was little nonspecific binding in the cortex.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes%20and%20rodentia)]

Biodistribution studies in rats showed a marked accumulation of the tracer in the striata with 0.6–0.8% injected dose per gram (%ID/g) at 15 min after injection of [^11^C]5-OH-DPAT (17). Haloperidol pretreatment (1 mg/kg, 15 min before radiotracer injection) effectively reduced specific binding of [^11^C]5-OH-DPAT to the striata. Significant nonspecific binding was observed in the cortical regions and cerebellum. [^11^C]-5-OH-DPAT showed higher striata/cerebellum ratios than ^11^C-labeled hydroxytetralin analogs, such as [^11^C]PPHT and [^11^C]ZYY-339.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes%20and%20%28primate%20not%20human%29)]

Mukherjee et al. (17) showed selective uptake in the striata (0.03% ID/ml) of rhesus monkeys with the striata/cerebellum ratios of 1.5 at 10 min and 2.0 at 60 min after injection of 111 MBq (3 mCi) of [^11^C]5-OH-DPAT. However, there was substantial nonspecific binding in the cortex. The authors suggested that use of the more active isomer may provide a higher striata/cerebellum ratio. [^11^C]-5-OH-DPAT showed higher striata/cerebellum ratios than ^11^C-labeled hydroxytetralin analogs, such as [^11^C]PPHT and [^11^C]ZYY-339.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-OH-DPAT%20and%20carbon%20radioisotopes%20and%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Sunahara R.K., Guan H.C., O'Dowd B.F., Seeman P., Laurier L.G., Ng G., George S.R., Torchia J., Van Tol H.H., Niznik H.B. (1991). Cloning of the gene for a human dopamine D5 receptor with higher affinity for dopamine than D1. Nature.
6 Sibley D.R., De Lean A., Creese I. (1982). Anterior pituitary dopamine receptors. Demonstration of interconvertible high and low affinity states of the D-2 dopamine receptor. J Biol Chem.
7 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
8 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
9 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
10 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
11 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
12 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2006). The striatal and extrastriatal d2/d3 receptor-binding profile of clozapine in patients with schizophrenia. Neuropsychopharmacology.
13 Kessler R.M., Ansari M.S., Riccardi P., Li R., Jayathilake K., Dawant B., Meltzer H.Y. (2005). Occupancy of striatal and extrastriatal dopamine d(2)/d(3) receptors by olanzapine and haloperidol. Neuropsychopharmacology.
14 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
15 Riccardi P., Li R., Ansari M.S., Zald D., Park S., Dawant B., Anderson S., Doop M., Woodward N., Schoenberg E., Schmidt D., Baldwin R., Kessler R. (2006). Amphetamine-induced displacement of [(18)f] fallypride in striatum and extrastriatal regions in humans. Neuropsychopharmacology.
16 Shi B., Narayanan T.K., Yang Z.Y., Christian B.T., Mukherjee J. (1999). Radiosynthesis and in vitro evaluation of 2-(N-alkyl-N-1'-11C-propyl)amino-5-hydroxytetralin analogs as high affinity agonists for dopamine D-2 receptors. Nucl Med Biol.
17 Mukherjee J., Narayanan T.K., Christian B.T., Shi B., Dunigan K.A., Mantil J. (2000). In vitro and in vivo evaluation of the binding of the dopamine D2 receptor agonist (11)C-(R,S)-5-hydroxy-2-(di-n-propylamino)tetralin in rodents and nonhuman primate. Synapse.